# ^99m^Tc-(N^α^His)Ac-(Arg-N-CH_3_)-Arg-Pro-(dimethyl-Tyr)-(tertary-Leu)-Leu

Chemical name: | ^99m^Tc-(N^α^His)Ac-(Arg-N-CH_3_)-Arg-Pro-(dimethyl-Tyr)-(tertary-Leu)-Leu
Abbreviated name: | ^99m^Tc-NT-XIX
Synonym:
Agent category: | Peptide
Target: | Neurotensin receptors (NTRs)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal\contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/110611243?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/110611242?ordinalpos=1&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=4923) for more information about neurotensin receptor 1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NT-XIX)]

Neurotensin (NT) is a tridecapeptide produced in the hypothalamus (1). It binds to NT receptors (NTRs) with high affinity and is implicated in the regulation of luteinizing hormone and prolactin release, and it has significant interaction with the dopaminergic system. There are three NTR subtypes, namely NTR1, NTR2, and NTR3. Most of the NT actions are mediated by NTR1, which is a G-protein–coupled receptor. The functions of NTR2 and NTR3 are not well known. The findings of NTR1 overexpression in various human tumors (2, 3), such as breast, lung, colon, pituitary, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the NTR1.

NT is rapidly metabolized in plasma by proteinases (4). Several NT analogs have been developed by modifications of the amino acid cleavage sites of NT(8-13) to increase plasma stability (5, 6). Maes et al. (6) has identified a modified peptide, (N^α^His)Ac-(Arg-N-CH_3_)-Arg-Pro-(dimethyl-Tyr)-(tertary-Leu)-Leu (NT-XIX), to be metabolically stable in plasma with good affinity for NTR1. ^99m^Tc-Labeled NT-XIX (^99m^Tc-NT-XIX) has been evaluated as a single-photon emission computed tomography (SPECT) imaging agent of NTR1 in nude mice bearing human colon adenocarcinoma HT-29 cells (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NT-XIX+synthesis)]

A solution of ^99m^Tc-pertechnetate, sodium boranocarbonate, borax, K-Na tartrate tetrahydrate, and sodium carbonate was heated for 20 min at 100°C (5). NT-XIX (20 nmol) was added to this cooled solution and heated for 60 min at 75°C. ^99m^Tc-NT-XIX was purified with high-performance liquid chromatography. The labeling yield was >95%. The specific activity of the purified product was not reported. ^99m^Tc-NT-XIX (0.2 pM) was >99% intact in human plasma after 24 h at 37°C with a half-life of 28 days.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NT-XIX+in+vitro)]

Garcia-Garayoa et al. (5) performed in vitro internalization studies of ^99m^Tc-NT-XIX in cultured HT-29 cancer cells at 37°C. HT-29 cells exhibited rapid internalization with 5.5% of radioactivity accumulated at 120 min after incubation. Approximately 50% of the internalized radioactivity remained inside the cells after 24 h of incubation. In vitro receptor-binding assays showed that the binding of ^99m^Tc-NT-XIX to the HT-29 cells was saturable with a binding constant (K_d_) value of 15 ± 6 nM (6). The K_d_ value for ^125^I-labeled NT was 1.6 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NT-XIX+rodentia)]

Garcia-Garayoa et al. (5) performed ex vivo biodistribution studies of 4 MBq (0.11 mCi) ^99m^Tc-NT-XIX in nude mice (n = 3/group) bearing HT-29 xenografts. Tumor accumulation was 5.9 ± 1.1% injected dose (ID)/g at 1.5 h, 5.2 ± 0.5% ID/g at 5 h, and 2.5 ± 0.2% at 24 h after injection. The organ with the highest uptake was the intestines (5.2 ± 0.5% ID/g), followed by the kidneys (~4.8% ID/g), liver (~3.0% ID/g), and stomach (~1.5% ID/g); little radioactivity (<1% ID/g) accumulated in the muscle, pancreas, blood, and bone at 1.5 h after injection. The half-life of ^99m^Tc-NT-XIX in blood from the injected mice was 1.4 h. Tumor/blood ratio was 13, 28, and 118 at 1.5, 5, and 24 h after injection, respectively. Co-administration of excess NT-XIX (0.3 mg/mouse) inhibited tumor accumulation by 78% at 1.5 h after injection, whereas accumulation in the intestines and stomach (NTR1-positive) was inhibited by 78% and 61%, respectively. Little effect was observed in the NTR1-negative tissues (kidneys, liver, pancreas, and muscle). SPECT imaging in nude mice bearing HT-29 xenografts was performed with 4 MBq (0.11 mCi) ^99m^Tc-NT-XIX. The tumors were clearly visualized at 1.5 h after injection. Co-administration of excess NT-XI substantially inhibited the radioactivity in the tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NT-XIX+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NT-XIX+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NT-XIX+human)]

No publication is currently available.

## References

1 Vincent J.P., Mazella J., Kitabgi P. (1999). Neurotensin and neurotensin receptors. Trends Pharmacol Sci.
2 Carraway R.E., Plona A.M. (2006). Involvement of neurotensin in cancer growth: evidence, mechanisms and development of diagnostic tools. Peptides.
3 Evers B.M. (2006). Neurotensin and growth of normal and neoplastic tissues. Peptides.
4 Kitabgi P., De Nadai F., Rovere C., Bidard J.N. (1992). Biosynthesis, maturation, release, and degradation of neurotensin and neuromedin N. Ann N Y Acad Sci.
5 Garcia-Garayoa E., Blauenstein P., Blanc A., Maes V., Tourwe D., Schubiger P.A. (2009). A stable neurotensin-based radiopharmaceutical for targeted imaging and therapy of neurotensin receptor-positive tumours. Eur J Nucl Med Mol Imaging.
6 Maes V., Garcia-Garayoa E., Blauenstein P., Tourwe D. (2006). Novel 99mTc-labeled neurotensin analogues with optimized biodistribution properties. J Med Chem.